# ^99m^Tc-(Hydrazinonicotinic acid-duramycin)(tricine)(TPPTS)

Chemical name: | ^99m^Tc-(Hydrazinonicotinic acid-duramycin)(tricine)(TPPTS)
Abbreviated name: | ^99m^Tc-Duramycin
Synonym:
Agent category: | Peptide
Target: | Phosphatidylethanolamine (PE)
Target category: | Binding
Method of detection: | SPECT, gamma planar imaging
Source of signal\contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+Duramycin)]

Apoptosis (programmed cell death) plays an important role in the pathophysiology of many diseases, such as cancer, neurodegenerative disorders, vascular disorders, and chronic hepatitis, as well as in the biology of normal cells, such as epithelial cells and immune cells (1). During apoptosis, there is rapid redistribution of phosphatidylserine (PS) and phosphatidylethanolamine (PE) from the inner membrane leaflet to the outer membrane leaflet, exposing the anionic head group.

Duramycin (Mw = 2 kDa) is a tetracyclic peptide of 19 amino acids that is produced by Streptoverticillium cinnamoneus and is closely related to cinnamycin (2, 3). Both compounds are lantibiotics, which are characterized by the presence of a high proportion of unusual amino acids. Both specifically bind PE, whereas annexin V (Mw = 32–35 kDa) binds to PS (4). PE and PS are present in the inner leaflet of plasma membrane, with little presence in the outer surface of normal viable cells (5). On the other hand, PS and PE are also accessible for binding in necrosis because of disruption of the plasma membrane. Annexin V binds to PS with high affinity (dissociation constant (K_d_) = 7 nM) (4), and duramycin binds to PE with a K_d_ value of 11 nM (6). Annexin V has been radiolabeled for imaging of apoptosis (7-9). Zhao et al. (10) have used a ternary ligand system (hydrazinonicotinic acid (HYNIC), tricine, and trisodium triphenylphosphine-3,3',3''-trisulfonate (TPPTS)) to label duramycin. HYNIC is a bifunctional coupling agent for ^99m^Tc labeling, whereas tricine and TPPTS are used as co-ligands to prepare the ternary ligand complex ^99m^Tc(HYNIC-duramycin)(tricine)(TPPTS) (^99m^Tc-duramycin) for single-photon emission computed tomography (SPECT) imaging of acute cell death in rats.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+Duramycin+synthesis)]

A solution (0.32 ml) of tricine (40 mg), SnCl_2_ (0.02 mg), TPPTS (1 mg), Na^99m^TcO_4_ (37 MBq (1 mCi)), and HYNIC-duramycin (0.015 mg) was incubated for 40 min at room temperature (10). The specific activity at end of synthesis was 58 GBq/mmol (1.57 Ci/mmol) with a radiochemical purity of 78-89% and a radiolabeling efficiency of 80–85%. ^99m^Tc-duramycin was purified with high-performance liquid chromatography. ^99m^Tc-duramycin was >97% intact after 2 h in the presence of 100-fold excess of cysteine.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+Duramycin+in+vitro)]

Apoptotic Jurkat T cells incubated with ^99m^Tc-duramycin exhibited ~32-fold higher binding than normal Jurkat T cells (10). Binding in the apoptotic cells was inhibited by PE-liposomes in a dose-dependent manner with a 50% inhibition concentration value of ~0.1 nM but not by liposomes that consisted of other phospholipid species.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+Duramycin+%20rodentia)]

Zhao et al. (10) performed biodistribution studies of ^99m^Tc-duramycin in normal rats (n = 4). The level of radioactivity was low in the blood with a half-life of <4 min. The organ with the highest uptake was the kidney (2.32 ± 0.48% injected dose (ID)/g) with little radioactivity in the other organs and tissues at 60 min after injection. Most of the injected radioactivity (22.1 ± 13.3% ID/g) was found in the urine sample at 60 min after injection. ^99m^Tc-duramycin was intact in the urine and blood samples at 60 min after injection. SPECT imaging in rats with acute myocardial infarction was performed with 7.4 MBq (0.2 mCi, 2.3 nmol) ^99m^Tc-duramycin. The infarcted area, kidneys, and urinary bladder were clearly visualized at 1 h after injection. Injection of inactivated ^99m^Tc-duramycin (modification of Asp15) showed an initial accumulation in the infarcted area with a rapid washout. Radioactivity at the infarcted area 1 h after injection was 4.0% ID/g for ^99m^Tc-duramycin and <1.0% ID/g for inactivated ^99m^Tc-duramycin. The accumulation of radioactivity in the infarcted tissues was confirmed with autoradiography and histology. No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+Duramycin+and%20%28pig%20or%20dog%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+Duramycin+and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+Duramycin+human)]

No publication is currently available.

## References

1 Thompson C.B. (1995). Apoptosis in the pathogenesis and treatment of disease. Science.
2 Marki F., Hanni E., Fredenhagen A., van Oostrum J. (1991). Mode of action of the lanthionine-containing peptide antibiotics duramycin, duramycin B and C, and cinnamycin as indirect inhibitors of phospholipase A2. Biochem Pharmacol.
3 Hayashi F., Nagashima K., Terui Y., Kawamura Y., Matsumoto K., Itazaki H. (1990). The structure of PA48009: the revised structure of duramycin. J Antibiot (Tokyo).
4 Reutelingsperger C.P., van Heerde W.L. (1997). Annexin V, the regulator of phosphatidylserine-catalyzed inflammation and coagulation during apoptosis. Cell Mol Life Sci.
5 Bevers E.M., Comfurius P., Dekkers D.W., Zwaal R.F. (1999). Lipid translocation across the plasma membrane of mammalian cells. Biochim Biophys Acta.
6 Iwamoto K., Hayakawa T., Murate M., Makino A., Ito K., Fujisawa T., Kobayashi T. (2007). Curvature-dependent recognition of ethanolamine phospholipids by duramycin and cinnamycin. Biophys J.
7 Blankenberg F.G. (2004). Recent advances in the imaging of programmed cell death. Curr Pharm Des.
8 Lahorte C., Slegers G., Philippe J., Van de Wiele C., Dierckx R.A. (2001). Synthesis and in vitro evaluation of 123I-labelled human recombinant annexin V. Biomol Eng.
9 Keen H.G., Dekker B.A., Disley L., Hastings D., Lyons S., Reader A.J., Ottewell P., Watson A., Zweit J. (2005). Imaging apoptosis in vivo using 124I-annexin V and PET. Nucl Med Biol.
10 Zhao M., Li Z., Bugenhagen S. (2008). 99mTc-labeled duramycin as a novel phosphatidylethanolamine-binding molecular probe. J Nucl Med.